# [^99m^Tc-Gly-Gly-Cys]-Ornithine-ornithine-ornithine-cyclo(Arg-Gly-Asp-D-Phe-Lys)

Chemical name: | [^99m^Tc-Gly-Gly-Cys]-Ornithine-ornithine-ornithine-cyclo(Arg-Gly-Asp-D-Phe-Lys)
Abbreviated name: | [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK)
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=23831237), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=56237028) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3678&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about integrin α_v_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=orn%20CGG%20RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled RGD analogs have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Dijkgraaf et al. (13) reported the development of ^111^In-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Glu-cyclo(Arg-Gly-Asp-D-Phe-Lys) (^111^In-DOTA-E-c(RGDfK)) for single-photon emission computed tomography (SPECT) imaging α_v_β_3_ receptors in nude mice bearing ovarian carcinoma tumors. Tsiapa et al. (14) prepared [^99m^Tc -Gly-Gly-Cys]-ornithine-ornithine-ornithine-cyclo(Arg-Gly-Asp-D-Phe-Lys) ([^99m^Tc-GGC]-(Orn)_3_-c(RGDfK)) as a radioligand for use in tumor imaging showing relatively high tumor accumulation and renal elimination with low abdominal accumulation in mice.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=orn%20CGG%20RGD+synthesis)]

Tsiapa et al. (14) prepared the synthesis of [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) by reacting GGC-(Orn)_3_-c(RGDfK) with 370–555 MBq (10–15 mCi) Na^99m^TcO_4_, sodium gluconate, sodium bicarbonate, and stannous chloride for 30 min at 37°C. [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) was purified with high-performance liquid chromatography. The radiochemical yield was >95%. The specific activity of [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) was not reported. [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) exhibited a log P_7.4_ value of −2.45 ± 0.01 (n = 3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=orn%20CGG%20RGD+in+vitro)]

[^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) remained 92.7% and 93.3% intact in the presence of 0.1 µM Cys for 60 min and 120 min (14), respectively, at 37ºC. [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) remained >90% intact in human plasma for 120 min at 37ºC.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=orn%20CGG%20RGD+rodentia)]

Tsiapa et al. (14) performed ex vivo biodistribution studies of 3.7 MBq (0.1 mCi) [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) at 5, 30, 60, and 120 min in nude mice (n = 3–5/group) bearing U87MG human glioblastoma tumors. The initial radioactivity accumulation in the U87MG tumors expressing the α_v_β_3_ integrin was 4.00 ± 0.05% injected dose (ID)/g at 5 min and decreased to 3.87 ± 0.48% ID/g at 60 min and 3.39 ± 1.05% ID/g at 120 min. At 60 min, the highest radioactive concentration was found in the kidney (72.17% ID/g), followed by the lung (2.27% ID/g), intestines (1.98% ID/g), liver (1.60% ID/g), and stomach (1.19% ID/g). Blood levels were 0.91% ID/g at 30 min and 0.88% ID/g at 60 min. Co-injection with excess c(RGDfK) (0.1 mg/mouse) reduced radioactivity accumulation by 70% in the tumors at 60 min. Maximum tumor/blood and tumor/muscle ratios were 4.39 at 60 min and 10.08 at 120 min, respectively.

Dynamic SPECT gamma planar imaging was performed in nude mice (n = 4) bearing U87MG tumors for 90 min after injection of 3.7 MBq (0.1 mCi) [^99m^Tc-GGC]-(Orn)_3_-c(RGDfK) (14). The tumors were clearly visualized as early as 5 min and at the end of 90 min scan with 6%–7% ID. The kidneys and urinary bladder exhibited 30%–40% ID and 25% ID during the 90-min scans. In one mouse with co-injection with excess c(RGDfK) the tumor was not visualized.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=orn%20CGG%20RGD+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=orn%20CGG%20RGD+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=orn%20CGG%20RGD+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Dijkgraaf I., Kruijtzer J.A., Frielink C., Corstens F.H., Oyen W.J., Liskamp R.M., Boerman O.C. (2007). Alpha v beta 3 integrin-targeting of intraperitoneally growing tumors with a radiolabeled RGD peptide. Int J Cancer.
14 Tsiapa I., Loudos G., Varvarigou A., Fragogeorgi E., Psimadas D., Tsotakos T., Xanthopoulos S., Mihailidis D., Bouziotis P., Nikiforidis G.C., Kagadis G.C. (2013). Biological evaluation of an ornithine-modified (99m)Tc-labeled RGD peptide as an angiogenesis imaging agent. Nucl Med Biol.